# ^64^Cu-1,4,7-Triazacyclononane-1,4-7-triacetic acid-8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane- triacetic acid-8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_
Abbreviated name: | ^64^Cu-NOTA-8-Aoc-BBN[7-14]NH_2_
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system and the gastrointestinal system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on central nervous system and gastrointestinal tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B (NMB) receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Prasanphanich et al. (7) used 1,4,7-triazacyclononane-1,4-7-triacetic acid (NOTA) as a bifunctional chelator for labeling 8-aminooctanoic acid-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_ (8-Aoc-BBN[7-14]NH_2_) with ^64^Cu. ^64^Cu-NOTA-8-Aoc-BBN[7-14]NH_2_ has been evaluated as a positron emission tomography (PET) imaging agent of GRPR in nude mice bearing human PC-3 prostate cancer cells.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+synthesis)]

8-Aoc-BBN[7-14]NH_2_ was prepared with solid-phase peptide synthesis with subsequent addition of NOTA group to form NOTA-8-Aoc-BBN[7-14]NH_2_ (7). ^64^CuCl_2_ was added to a solution of NOTA-8-Aoc-BBN[7-14]NH_2_ in ammonium acetate (pH 7.0). The mixture was heated for 60 min at 70°C. The product, ^64^Cu-NOTA-8-Aoc-BBN[7-14]NH_2_, was purified with high-performance liquid chromatography with a yield of >90% and a radiochemical purity of >99%. The specific activity of ^64^Cu-NOTA-8-Aoc-BBN[7-14]NH_2_ was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+in+vitro)]

Prasanphanich et al. (7) performed in vitro inhibition studies of NOTA-8-Aoc-BBN[7-14]NH_2_ in cultured human prostate PC-3 tumor cells with ^125^I-BBN. The 50% inhibition concentration (IC_50_) value was 3.1 ± 0.5 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+%20rodentia)]

Prasanphanich et al. (7) performed ex vivo biodistribution studies of 0.26 MBq (7 μCi) ^64^Cu-NOTA-8-Aoc-BBN[7-14]NH_2_ in normal mice. The heart, lung, spleen, stomach, muscle, bone, brain, and blood exhibited very little (<0.5% injected dose per gram (ID/g)) of the accumulated conjugate at 1, 4, and 24 h after injection. Pancreatic accumulation was 27.0 ± 3.2, 9.1 ± 1.4, and 1.42 ± 0.13% ID/g at the respective time points. The small intestine showed accumulation of 10.8 ± 1.1, 1.87 ± 0.51, and 0.37 ± 0.06% ID/g, while the large intestine accumulated 2.14 ± 0.35, 15.1 ± 3.9, and 0.53 ± 0.16% ID/g at these time points. Radioactivity accumulation in the kidney was 2.92 ± 0.64, 0.72 ± 0.07, and 0.42 ± 0.05% ID/g, respectively. Accumulation in the liver was 1.54 ± 0.59, 1.07 ± 0.10, and 0.73 ± 0.09% ID/g, respectively. The urinary excretion was 76% ID at 4 h after injection. Administration of D-lysine (15 mg/mouse) had little effect on the biodistribution of ^64^Cu-NOTA-8-Aoc-BBN[7-14]NH_2_. Ex vivo biodistribution studies of ^64^Cu-NOTA-8-Aoc-BBN[7-14]NH_2_ were performed in nude mice bearing PC-3 xenografts. Tumor accumulation at these time points was 3.59 ± 0.70 and 1.00 ± 0.19% ID/g, while the biodistribution pattern in the other tissues was similar to that of the normal mice. The tumor/muscle ratios were 9.5, 7.5, and 5.6 at 1, 4, and 24 h after injection, respectively. Pretreatment with excess BBN[1-14] (100 µg/mouse) inhibited the tumor accumulation by 40%, whereas the accumulation in the pancreas and intestines at 1 h after tracer injection was inhibited by 95% and 75%, respectively. Little effect was observed in the other tissues. PET imaging in nude mice bearing PC-3 xenografts was performed with 55.5 MBq (1.5 mCi) ^64^Cu-NOTA-8-Aoc-BBN[7-14]NH_2_ at 24 h after injection. The tumors were clearly visualized, as were the pancreas, liver, and kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+NOTA+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Prasanphanich A.F., Nanda P.K., Rold T.L., Ma L., Lewis M.R., Garrison J.C., Hoffman T.J., Sieckman G.L., Figueroa S.D., Smith C.J. (2007). [64Cu-NOTA-8-Aoc-BBN(7-14)NH2] targeting vector for positron-emission tomography imaging of gastrin-releasing peptide receptor-expressing tissues. Proc Natl Acad Sci U S A.